# 2-Deoxy-2-[^18^F]fluorosorbitol

Chemical name: | 2-Deoxy-2-[^18^F]fluorosorbitol
Abbreviated name: | [^18^F]FDS
Synonym:
Agent Category: | Compound
Target: | Brain tumors and inflammation
Target Category: | Cellular accumulation after phosphorylation
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS&WebEnv=0058mgFn4gXJzYv0MEfCxVRB7RSwMgUdCSlpTwotQa1ayi5SMIvUDM_932ntRsALCOYATcBqNAvKM%407748428072881B60_0000SID&WebEnvRq=1)]

The glucose analog 2-deoxy-2-[^18^F]fluoro-D-glucose ([^18^F]FDG) is a recommended radiochemical that is often used for the detection and posttherapy monitoring of commonly occurring cancers such as Hodgkin’s disease and non-Hodgkin’s lymphoma (1). The ^18^F-labeled FDG is transported into the cell by the glucose transporters, is phosphorylated, and remains trapped in the cell without further metabolism. So, this glucose analog can be used to monitor the uptake of glucose by the cells, but it can not be used to track glucose metabolism within the cell (2). Neoplastic cells are highly proliferative and have a high rate of glucose metabolism compared to normal tissue, and they tend to accumulate [^18^F]FDG, which can be used to detect and monitor various cancerous lesions by positron emission tomography (PET) (3, 4). In addition, glucose is the main source of energy for the brain because this tissue has a very high concentration of neurons that can not metabolize free fatty acids (5). However, because [^18^F]FDG produces high background interference in the brain, it is difficult to detect cancerous lesions in the brain tissue with this radiochemical (6).

Li et al. have evaluated the use of 2-deoxy-2-[^18^F]fluorosorbitol ([^18^F]FDS) for the detection of lesions that are not easily detected with [^18^F]FDG, particularly in the brain (6). This was based on the fact that FDS is structurally similar to glucose, does not use the glucose transport system for entry into cells, probably is not metabolized in the brain, and can be synthesized easily by the reduction of FDG (7). This chapter describes the in vitro and in vivo imaging studies carried out with [^18^F]FDS.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS+synthesis&WebEnv=0LRqGB9Y1EK-m5thqiI2mF5CfQOVTSBT6mxvqy_Q61PYwm2urgk3fL6gVQJfl8qH6jBVV_E5zI3uqs%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of [^18^F]FDS was described by Li et al. (6). Briefly, sodium borohydride was added to a solution of [^18^F]FDG in saline. The mixture was stirred at 35°C for 15 min. The reaction was quenched (the investigators did not describe how the reaction was quenched), and the pH was adjusted to 7.4. The mixture was subsequently filtered through an Alumina-N Sep-Pak cartridge, and the filtrate was analyzed by radio thin-layer chromatography. Using acetonitrile and water as the eluent for thin-layer chromatography, the Rf values for [^18^F]FDS and [^18^F]FDG were 0.33 and 0.54, respectively. The total time required for the synthesis was ~30 min with a yield (decay-corrected) of 81 ± 4%. Based on [^18^F]FDG, the specific activity of [^18^F]FDS was reported to be 100–200 TBq/mmol (270–540 Ci/mmol). The investigators did not report the stability of the labeled product (6).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS+in+vitro&WebEnv=0bEyUOJHmRZO7Txen9rqDsaFEGeUIRZZyD3wGdoOdAti5Cf4z3nZExnLIlDmOlH6lt_aVkGUcc4YPR%407748428072881B60_0000SID&WebEnvRq=1)]

The uptake and efflux of [^18^F]FDS and [^18^F]FDG were compared with U87MG (http://www.biotech.ist.unige.it/cldb/cl4592.html) cells, a glioblastoma-astrocytoma cell line (6). To determine the uptake of [^18^F]FDS and [^18^F]FDG, the cells were respectively exposed to the radiochemicals for 10–180 min in glucose-free medium, and the cells were lysed after washing to determine the accumulation of radioactivity. For the efflux study, the cells were respectively exposed to the radiochemicals for 180 min as described above and then washed to remove the labeled compounds from the growth medium. The cells were then recultured in glucose-free medium for 15–180 min, washed with the same medium, and lysed to determine the accumulated radioactivity. Approximately 40% of the total [^18^F]FDG was taken up by the cells, whereas only ~0.1% of the total [^18^F]FDS accumulated in the cells. A rapid efflux of [^18^F]FDS from the cells, which reached equilibrium in ~10 min, was observed. However, with [^18^F]FDG the efflux was gradual and did not reach equilibrium even after 180 min. Although [^18^F]FDG uptake by the U87MG cells was influenced significantly by the presence of glucose (it decreased the uptake) or insulin (it increased the uptake), no such effect was observed with either agent on the [^18^F]FDS uptake by these cells (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS+rodentia&WebEnv=0J3aK0uQyJtWIkFZeISHlVesDVmFP68ZrHXkZGVS9FAaKBxIGyO-kwQGmp1RtgIz2uuvhJOWAYY-Kx%407748428072881B60_0000SID&WebEnvRq=1)]

PET studies were performed with [^18^F]FDS and [^18^F]FDG in a murine model of mice either bearing xenograft tumors or after the induction of inflammation (6). To generate the xenograft tumors, U87MG cells were injected either subcutaneously in the front legs or intracranially in athymic mice (n = 3 mice per time point), and the tumors were allowed to engraft for 3–4 or 6–7 weeks, respectively. In another study, glioma tumors were generated with intracranial injections of highly tumorogenic GL-26 cells (originally from the National Cancer Institute, Bethesda, Maryland) in syngenic C57BL/6 mice (n = 3 mice per time point) as described above; the mice were subjected to PET imaging 25–30 days after tumor inoculation. The mice were injected with radioactive FDG or FDS, and the PET images were obtained at different time points for the tumor and the major organs (liver, heart muscle, intestines, and kidneys). The U87MG tumor uptake was calculated to be 2.43% of the injected dose/gram tissue (% ID/g) at 15 min after injection, and the tumor/major organ ratios were also determined. From these ratios it was evident that [^18^F]FDS was a suitable tracer to detect brain lesions because it had a tumor/brain ratio of up to 13.6 compared to ratio of 0.5–4.5 for the other organs. Compared to [^18^F]FDS, the uptake of [^18^F]FDG was high in both the U87MG tumors and the normal brain tissue (6). In the GL-26 model, a high uptake of [^18^F]FDS (6.38% ID/g) was also observed in the tumors, which were clearly visible with this radiochemical. In comparison, [^18^F]FDG was unable to distinguish between the neoplastic and normal tissue in the brain.

To induce inflammation, a solution of 12-O-tetradecanoyl-phorbol-13-acetate (TPA) in acetone was applied to the inner and outer surfaces of the right ears of three BALB/c mice (6). The untreated left ear served as the control for each animal. An edematous swelling was noted within 6 h of TPA application on the right ear, at which point the mice were subject to PET imaging after the administration of either [^18^F]FDG or [^18^F]FDS. Both labeled compounds showed a higher accumulation in the inflamed ear compared to the control ear. Although the accumulation of radioactivity was higher for [^18^F]FDG compared to [^18^F]FDS, with a right ear/left ear uptake ratio of 3.44 ± 0.25, the uptake ratio was higher (4.21 ± 1.33) for the labeled sorbitol derivative. The investigators reported that it was more difficult to detect the inflamed ear with [^18^F]FDG versus [^18^F]FDS using PET because of the interference of high brain activity (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS+Non-Primate+Mammals&WebEnv=0OQoCZ6mILGQYe0dLZfxhE7RAHJcoskkIFLuH_QiqRvCKscYYYeUePtDcBJZXNyiQ3K9noGbQo39oE%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS+Non+Human+Primates&WebEnv=0pVJq34IvjKmyYh44loTxA_Uet2SUHCtsuTnjJ2CzvGF8Et9PznjkOM9iedduYzh2qLhFJnf091pe2%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FDS+Humans&WebEnv=0aLrQ46VWuOSNN9G5i8xV1FMZQfFAWPUxM6hK7ai6sgWPC9BEZYFR5ET2b2I7dqKbk4H0ov5wYTTkD%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Some studies reported in this chapter were funded by NCI grants R01 CA119053, R21 CA121842, R21 CA102123, ICMIC P50 CA114747, CCNE U54 CA119367, and R24 CA93862.

## References

1 Juweid M.E. (2008). 18F-FDG PET as a Routine Test for Posttherapy Assessment of Hodgkin's Disease and Aggressive Non-Hodgkin's Lymphoma: Where Is the Evidence?. J Nucl Med.
2 Smith T.A. (2001). The rate-limiting step for tumor [18F]fluoro-2-deoxy-D-glucose (FDG) incorporation. Nucl Med Biol.
3 Brahimi-Horn M.C., Pouyssegur J. (2007). Hypoxia in cancer cell metabolism and pH regulation. Essays Biochem.
4. Chung, H.H., W.J. Kang, J.W. Kim, N.H. Park, Y.S. Song, J.K. Chung, and S.B. Kang, The clinical impact of [(18)F]FDG PET/CT for the management of recurrent endometrial cancer: correlation with clinical and histological findings. Eur J Nucl Med Mol Imaging, 2008.
5 Tomlinson D.R., Gardiner N.J. (2008). Glucose neurotoxicity. Nat Rev Neurosci.
6. Li, Z.B., Z. Wu, Q. Cao, D.W. Dick, J.R. Tseng, S.S. Gambhir, and X. Chen, The Synthesis of (18)F-FDS and Its Potential Application in Molecular Imaging. Mol Imaging Biol, 2007.
7 Scott M.E., Viola R.E. (1998). The use of fluoro- and deoxy-substrate analogs to examine binding specificity and catalysis in the enzymes of the sorbitol pathway. Carbohydr Res.